# ^99m^Tc-Arcitumomab

Chemical name: | ^99m^Tc-Arcitumomab
Abbreviated name: | ^99m^Tc-IMMU-4
Synonym: | CEA-Scan^®^, ^99m^Tc-NP-4 anti-CEA MAb Fab´
Agent Category: | Antibody
Target: | Carcinoembryonic antigen (CEA)
Target Category: | Antibody to antigen binding
Method of detection: | Single Photon Emission Computed Tomography (SPECT), planar imaging
Source of signal/contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=180211), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=29856) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=5670) for more information about CEA.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D)]

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2899mTc-IMMU-4%20or%20Arcitumomab%20or%20CEA%20Scan%29)]

^99m^Tc-Arcitumomab (^99m^Tc-IMMU-4), which is formed by the conjugation of ^99m^Tc with a murine anti-carcinoembryonic antigen (CEA) monoclonal antibody (MAb) Fab´ fragment, can be used for imaging CEA-expressing cancers (1). It was approved (http://www.cea-scan.com/main.htm) by the United States Food and Drug Administration (FDA) in 1999 as a diagnostic aid, in conjunction with standard diagnostic evaluations, for detection of the presence, location, and extent of recurrent and/or metastatic colorectal carcinoma involving the liver, extrahepatic abdomen, and pelvis in patients with a histologically confirmed diagnosis of colorectal carcinoma (2). However, it is no longer marketed (http://www.cea-scan.com/main.htm) in the United States. ^99m^Tc-IMMU-4 is not indicated for the differential diagnosis of suspected colorectal carcinoma or as a screening tool for colorectal cancer, nor is it intended for readministration or for assessment of response to treatment.

CEA was first identified from extracts of human adenocarcinoma of the colon (3). It is a β-glycoprotein, and its predominant expression on the cell surface is increased in a variety of carcinomas, particularly of the gastrointestinal tract, as well as in fetal gastrointestinal tissues and in certain inflammatory states, such as inflammatory bowel disease (1, 4). CEA, which exhibits extensive heterogeneity in its physicochemical and immunologic properties (3, 5), has a molecular weight of 200 kDa, and can be shed and detected in the serum (5). It has been used as a serum marker for monitoring disease status in patients who have various CEA- secreting tumors (gastrointestinal, lung, medullary, thyroid, uterine, ovarian, and bladder carcinomas). Other cross-reactive, but genetically distinct, CEA variants have been identified, including nonspecific cross-reactive antigen (NCA) and meconium antigen (MA) (2).

Radiolabeled MAbs have been developed for both the diagnosis and treatment of tumors (4). IMMU-4 was developed from the anti-CEA NP-4 MAb (2, 5, 6). NP-4, a murine IgG_1K_ MAb, binds only CEA and does not appear to cross-react with NCA or MA. IMMU-4 is obtained from NP-4 in the form of a 50-kDa monovalent Fab´ fragment, by pepsin digestion and is devoid of the immunogenic Fc portion (7). This improves the imaging pharmacokinetics of IMMU-4 by allowing faster clearance from the blood pool and other soft tissues, reducing liver metabolism, and improving the tumor/background ratio. Being a smaller molecule, the Fab´ fragment also minimizes induction of human anti-mouse antibodies (HAMAs) in patients.

MAbs can be labeled with ^99m^Tc by direct or indirect labeling. Direct labeling involves reduction of ^99m^Tc pertechnetate and nonspecific binding of the reduced ^99m^Tc to donor atoms, namely, thiol, amide, amino, and carboxylate (8). Indirect labeling uses a bifunctional chelating agent, which can be more binding site specific on the MAb molecule. IMMU-4 has also been labeled with radioactive iodine (9). In the FDA-approved product, IMMU-4 is directly labeled with ^99m^Tc by use of a reducing agent.

The IMMU-4 MAb in commercial preparations is produced in murine ascites fluid and is supplied as a lyophilized formulation that contains 1.25 mg of IMMU-4.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

NP-4 MAb was initially produced by Primus and colleagues in 1983 with use of the hybridoma technique and CEA isolated from liver metastases of a colonic adenocarcinoma (2, 5) NP-4 MAb was produced in mice and purified from ascites fluid by protein A and ion-exchange column chromatography at 4 ^o^C (10). It was cleaved with pepsin to produce F(ab´)_2_, and subsequently reduced to Fab´ as IMMU-4. Linder et al. (11) reported an indirect ^99m^Tc labeling method that uses BATO (boronic acid adduct of technetium dioximes) complexes as the bifunctional chelating agent to label NP-4 whole antibody and NP-4 F(ab’)_2_ antibody fragments. Building on earlier work (12), Hansen et al. (10) developed an instant ^99m^Tc-labeling kit for IMMU-4, using the direct labeling method. After lyophilizing the IMMU-4 with the reagents required for reduction of ^99m^Tc-pertechnetate, they stored the freeze-dried mixture at 4-8 ^o^C. To 1 mg of the lyophilized IMMU-4 form, they added 740 MBq (20 mCi) of ^99m^Tc-pertechnetate solution. The pertechnetate was reduced, and the ^99m^Tc was bound to the IMMU-4 Fab´ fragment. High-performance liquid chromatography (HPLC) analysis of the ^99m^Tc-IMMU-4 indicated that ~ 90-95% of the radioactivity was associated with monomeric Fab´. The bulk of the remaining radioactivity was associated with F(ab’)_2_. In the commercial preparation, 1.25 mg of Fab´ fragment is lyophilized with 0.29 mg of stannous chloride as a pertechnetate-reducing agent. The IMMU-4 is directly labeled with ^99m^Tc by reconstitution of the lyophilized MAb with 1110 MBq (30 mCi) of ^99m^Tc sodium pertechnetate in 1 ml of 0.9% sodium chloride. The radiolabeling reaction is completed within 5 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

Primus et al. (5) produced NP-4 anti-CEA MAb and performed in vitro studies of ^99m^Tc-IMMU-4. Using the competitive radioimmunoassay method, they obtained an affinity constant (K) of 8.9 х 10^8^ M−^1^. NP-4 did not bind to MA and NCA. Hansen et al. (10) evaluated the in vitro stability of ^99m^Tc-IMMU-4 prepared from the instant labeling kit by incubating the radiolabeled product in saline or 1-6% human serum albumin at 37 ^o^C for 24 h. Only 11% of the radioactivity was dissociated as ^99m^Tc pertechnetate after 24 h of incubation, and less than 10% was transferred to albumin. No loss of activity was observed when ^99m^Tc-IMMU-4 was challenged with a 2000-fold molar excess of diethylenetriaminepentaacetic acid for 4 h at room temperature. They also studied the stability of lyophilized IMMU-4. As measured by chromatography with a CEA affinity column, the immunoreactivity of ^99m^Tc-IMMU-4 prepared from the lyophilized vials did not change over 6 to 8 months.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28CEA%20Scan%20or%20Arcitumomab%20or%2099mTc-IMMU-4%29%20AND%20rodentia)]

Hansen et al. (10) performed biodistribution and imaging studies of ^99m^Tc-IMMU-4 in normal and athymic nude mice bearing a s.c. human colonic cancer, GW-39. Each mouse was given 10 µg of ^99m^Tc-IMMU4 by tail vein injection. The specific activity was 740 MBq/mg (20 mCi/mg) or 37 GBq/µmol (1 Ci/µmol) based on a molecular weight of 50 kDa for the Fab’ fragment. In normal mice without tumors, primary elimination of Tc-IMMU-4 was by the kidneys with 110.20 ± 16.04% injected dose (%ID)/g at 1 h and 49.44 ± 11.26% ID/g at 24 h after injection. The blood radioactivity decreased from 9.44 ± 1.50% ID/g at 1 h to 2.25 ± 0.24% ID/g and 0.35 ± 0.02% ID/g at 4 h and 24 h, respectively. The liver radioactivity was 4.37 ± 0.90% ID/g and 1.13 ± 0.15% ID/g at 1 h and 24 h, respectively. The lungs had 5.31 ± 0.69% ID/g and 0.56 ± 0.10% ID/g at 1 h and 24 h, respectively. No significant radioactivity was observed in the stomach, spleen, large intestine, or small intestine up to 20 h after injection. The biodistribution of ^99m^Tc-IMMU-4 in tumor bearing mice was similar to that in normal mice. The radioactivities at 2 h for the blood, liver, lungs and kidneys were 6.50 ± 0.91, 3.80 ± 0.80, 4.69 ± 0.81, and 91.60 ± 8.71% ID/g, respectively, and the radioactivities at 24h were 0.63 ± 0.16, 1.10 ± 0.15, 0.66 ± 0.40, and 28.68 ± 1.66% ID/g, respectively The tumor had 5.78 ± 0.56% ID/g at 2 h and 3.25 ± 0.41% ID/g at 24 h. The imaging study also demonstrated that the route of elimination of ^99m^Tc-IMMU-4 was urinary excretion. Tumor CEA-producing carcinomas outside the blood pool could be imaged by 2 h after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

Put non-primate mammals here.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

Put non-human primates here.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28CEA%20Scan%20or%20Arcitumomab%20or%2099mTc-IMMU-4%29%20AND%20human)]

Behr et al. (13) compared the metabolism and kinetics of ^99m^Tc-IMMU-4 (92% Fab´ fragment) with ^99m^Tc-labeled intact whole anti-CEA antibody (BW 431/26) and with a 79%/21% mixture of ^99m^Tc-labeled anti-CEA F(ab´)_2_/Fab´ fragment (F023C5) in 127 patients who had recurrent or primary colorectal carcinoma. The whole-body clearance of the fragments (^99m^Tc-F023C5, and ^99m^Tc-IMMU-4) was significantly higher (P < 0.001) than that of ^99m^Tc-BW 431/26. The whole-body retentions of ^99m^Tc-IMMU-4, ^99m^Tc-F023C5, and ^99m^Tc-BW 431/26 at 24 h were 67.5 ± 9.3, 64.4 ± 14.8, and 92.2 ± 7.4%, respectively. Significant differences were observed between the three ^99m^Tc-MAbs with respect to their serum clearance rates. The serum t_½_s for BW 431/26, F023C5 and IMMU-4 were 36, 8 and 4 h, respectively. The intact antibody BW 431/26 had a higher liver uptake with 15.6 ± 4.7%ID after 24 h, whereas F023C5 and IMMU-4 had 8.2 ± 3.8%ID and 10.0 ± 6%ID, respectively. In contrast, the kidney radioactivities at 24 h for IMMU-4, F023C5, and BW 431/26 were 18.4 ± 6.2%ID, 17.2 ± 7.2%ID, and 9.8 ± 4.2%ID, respectively. Gall bladder visualization was observed after 24 h only for the fragments, IMMU-4 and F023C5, but not for the intact MAb, BW 431/26. In imaging, the sensitivities of detecting liver metastases for ^99m^Tc-IMMU-4, ^99m^Tc-F023C5, and ^99m^Tc-BW 431/26 were 80% (n = 15), 72.5% (n = 40), and 44.1% (n = 68), respectively. However, the tumor/background radioactivity ratios of ^99m^Tc-IMMU-4, ^99m^Tc-F023C5, and ^99m^Tc-BW 431/26 were actually 1.43 ± 0.53, 1.29 ± 0.11, and 1.78 ± 0.29. This indicated that the higher sensitivity of detecting liver metastases with smaller fragments was a result of more rapid clearance of nonspecific activity.

In two prospective, open-label, phase III clinical trials of ^99m^Tc-IMMU-4, 210 presurgical patients with advanced recurrent or metastatic colorectal carcinomas were studied (14). ^99m^Tc-IMMU-4 scans (planar and single photon emission tomorgraphy (SPECT)) began at 2 to 5 h and then again at 18 to 24 h after i.v. injection of 555 MBq to 925 MBq (15 to 25 mCi) in 1 mg of IMMU-4. The overall imaging statistics for ^99m^Tc-IMMU-4 in terms of accuracy, sensitivity, specificity, positive predictive value (PPV), and negative predictive value (NPV) were 70, 71.3, 62.5, 91.4, and 28.2%, respectively. In comparison, the values for the conventional imaging modalities (conventional diagnostic methods (CDM) included, e.g., computed tomography, and chest X-ray) were 61.9, 57.9, 84.4, 95.4, and 26.5%, respectively. In 88 patients with occult disease, for whom the only evidence of disease recurrence was abnormal serum CEA, liver enzymes, or symptoms and signs, ^99m^Tc-IMMU-4 imaging combined with CDM appeared to increase the accuracy from 33% with CDM alone to 61%. Only minor side effects were observed, and two patients developed HAMAs after a single injection. None of the 19 patients developed HAMA after receiving 2 doses, and there was no morbidity attributed to circulating antigen-antibody complexes. Other studies appeared to support the clinical use of ^99m^Tc-IMMU-4 for radioimmunodetection of colorectal carcinoma [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28CEA%20Scan%20or%20Arcitumomab%20or%2099mTc-IMMU-4%29%20AND%20human%20AND%20colorectal%20carcinoma)] In two separate, small studies (28 patients in both studies) (15, 16), SPECT imaging with ^99m^Tc-IMMU-4 was found to be useful but not as sensitive as [^18^F]fluoro-2-deoxy-2-D- glucose ([^18^F]FDG) PET imaging to detect distant metastases and predict unresectable disease.

Wegener et al. (17) studied the efficacy and safety of repeated administration of ^99m^Tc-IMMU-4 in 44 patients. The imaging results after the second dose were comparable to those after a single injection. Only one adverse event, eosinophilia, was found to be related to ^99m^Tc-IMMU-4 injection. In all patients, no elevated HAMA titers and no significant hematology and serum chemistry changes were observed.

Radiation dosimetry (2) for ^99m^Tc-IMMU-4 showed that the highest dose was to the kidneys with 100 µGy/MBq (370 mrad/mCi). The doses to the bladder, spleen, liver, bone marrow, lung and ovaries were 16.6 µGy/MBq (61.5 mrad/mCi), 15.9 µGy/MBq (58.9 mrad/mCi), 10.4 µGy/MBq (38.5 mrad/mCi), 9.9 µGy/MBq (36.7 mrad/mCi), 7.7 µGy/MBq (28.5 mrad/mCi), and 7.7 µGy/MBq (28.5 mrad/mCi), respectively.

## NIH Support

USPHS Grant CA39841, NIH N44-BM-87778.

## References

1 Wahl R.L., Philpott G., Parker C.W. (1983). Monoclonal antibody radioimmunodetection of human-derived colon cancer. Invest Radiol.
2 (1999). . CEA-Scan (Arcitumomab) for the preparation of Tc 99m Arcitumomab, Immunomedics, Inc. p. 1-15.
3 Gold P., Freedman S.O. (1964). Demonstration of tumor-specific antigens in human colonic carcinomata by immunological tolerance and absorption techniques. The Journal of Experimental Medicine.
4 Kowalsky R.J., Falen S.W. (2004). and Radiopharmaceuticals in nuclear pharmacy and nuclear medicine, American Pharmacists Association: Washington, D.C. p. 733-752.
5 Primus F.J., Freeman J.W., Goldenberg D.M. (1983). Immunological heterogeneity of carcinoembryonic antigen: purification from meconium of an antigen related to carcinoembryonic antigen. Cancer Res.
6 Griffiths G.L. Goldenberg D.M. Roesch F. Hansen H.J. Radiolabeling of an anti-carcinoembryonic antigen antibody Fab' fragment (CEA-Scan) with the positron-emitting radionuclide Tc-94m Clin Cancer Res 1999 5Suppl10 3001s 3003s 10541334
7 Goldenberg D.M., Juweid M., Dunn R.M., Sharkey R.M. (1997). Cancer imaging with radiolabeled antibodies: new advances with technetium-99m-labeled monoclonal antibody Fab' fragments, especially CEA-Scan and prospects for therapy. J Nucl Med Technol.
8 Fritzberg A.R., Berninger R.W., Hadley S.W., Wester D.W. (1988). Approaches to radiolabeling of antibodies for diagnosis and therapy of cancer. Pharm Res.
9 Losman M.J., Hansen H.J., Sharkey R.M., Goldenberg D.M., Monestier M. (1991). Human response against NP-4, a mouse antibody to carcinoembryonic antigen: human anti-idiotype antibodies mimic an epitope on the tumor antigen. Proc Natl Acad Sci U S A.
10 Hansen H.J. Jones A.L. Sharkey R.M. Grebenau R. Blazejewski N. Kunz A. Buckley M.J. Newman E.S. Ostella F. Goldenberg D.M. Preclinical evaluation of an "instant" 99mTc-labeling kit for antibody imaging Cancer Res 1990 50Suppl3 794s 798s 2297726
11 Linder K.E., Wen M.D., Nowotnik D.P., Ramalingam K., Sharkey R.M., Yost F., Narra R.K., Nunn A.D., Eckelman W.C. (1991). Technetium labeling of monoclonal antibodies with functionalized BATOs: 2. TcCl(DMG)3CPITC labeling of B72.3 and NP-4 whole antibodies and NP-4 F(ab')2. Bioconjug Chem.
12 Hansen H.J., Jones A.L., Grebenau R., Kunz A., Goldenberg D.M. (1990). Labeling of anti-tumor antibodies and antibody fragments with Tc-99m. Cancer Treat Res.
13 Behr T. Becker W. Hannappel E. Goldenberg D.M. Wolf F. Targeting of liver metastases of colorectal cancer with IgG, F(ab')2, and Fab' anti-carcinoembryonic antigen antibodies labeled with 99mTc: the role of metabolism and kinetics Cancer Res 1995 55Suppl23 5777s 5785s 7493346
14 Moffat F.L., Pinsky C.M., Hammershaimb L., Petrelli N.J., Patt Y.Z., Whaley F.S., Goldenberg D.M. (1996). Clinical utility of external immunoscintigraphy with the IMMU-4 technetium-99m Fab' antibody fragment in patients undergoing surgery for carcinoma of the colon and rectum: results of a pivotal, phase III trial. The Immunomedics Study Group. J Clin Oncol.
15 Libutti S.K., Alexander H.R., Choyke P., Bartlett D.L., Bacharach S.L., Whatley M., Jousse F., Eckelman W.C., Kranda K., Neumann R.D., Carrasquillo J.A. (2001). A prospective study of 2-[18F] fluoro-2-deoxy-D-glucose/positron emission tomography scan, 99mTc-labeled arcitumomab (CEA-scan), and blind second-look laparotomy for detecting colon cancer recurrence in patients with increasing carcinoembryonic antigen levels. Ann Surg Oncol.
16 Willkomm P., Bender H., Bangard M., Decker P., Grunwald F., Biersack H.J. (2000). FDG PET and immunoscintigraphy with 99mTc-labeled antibody fragments for detection of the recurrence of colorectal carcinoma. J Nucl Med.
17 Wegener W.A., Petrelli N., Serafini A., Goldenberg D.M. (2000). Safety and efficacy of arcitumomab imaging in colorectal cancer after repeated administration. J Nucl Med.